# IRDye800-Anti-vascular endothelial growth factor receptor-2 monoclonal antibody Avas12a1

Chemical name: | IRDye800-Anti-vascular endothelial growth factor receptor-2 monoclonal antibody Avas12a1
Abbreviated name: | IRDye800-Avas12a1, NIR800-αVEGFR2ab
Synonym:
Agent category: | Antibody
Target: | Vascular endothelial growth factor receptor-2 (VEGFR-2)
Target category: | Receptor
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | IRDye 800CW
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=NP_002244), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NG_012004) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=3791) for more information about VEGFR-2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2%20optical)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive complement to radionuclide imaging in small animals.

Vascular endothelial growth factor (VEGF) consists of at least six isoforms of various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (4). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (5). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (4).

VEGF receptors were found to be overexpressed in various tumor cells and tumor-associated endothelial cells (6). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (7, 8). Radiolabeled VEGF tracers have been developed for imaging solid tumors and angiogenesis in humans (9-11). Virostko et al. (12) conjugated the monoclonal antibody Avas12a1 (rat anti-mouse VEGFR-2) with NIR dye IRDye 800CW as IRDye800-Avas12a1 for NIR imaging of VEGFR expression in vivo to study tumor angiogenesis.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=VEGFR+AND+micad%5Bbook%5D)
- Gene information in NCBI (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=3791))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=VEGFR)
- Clinical trials (VEGFR (http://www.clinicaltrials.gov/ct2/results?term=VEGFR))
- FDA Drug information (VEGFR (http://google2.fda.gov/search?q=VEGFR&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2%20optical+synthesis)]

Virostko et al. (12) prepared IRDye800-Avas12a1 by addition of N-hydroxyl-succimide ester of IRDye 800CW to Avas12a1 antibody at 4°C in 10:1 dye/antibody molar ratio. The mixture was incubated at room temperature for 3 h. IRDye800-Avas12a1 was purified with dialysis. The dye/antibody ratio was ~1 as determined with spectroscopy. IRDye800-Avas12a1 exhibited peak absorbance at 777 nm and fluorescence emission peak at 798 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2%20optical+in+vitro)]

In vitro binding studies were performed using mouse endothelial (bEnd3) cells expressing VEGFR-2 with IRDye800-Avas12a1 and non-targeted IRDye800-IgG (12). NIR fluorescence intensity was measured in bEnd3 cells after incubation with 40-1000 nM of for 30 min. There were 1-2 fold greater signal intensity in bEnd3 cells incubated with IRDye800-Avas12a1 than with IRDye800-IgG. Pretreatment with 400 nM Avas12a1 30 min prior to the addition of 40 nM IRDye800-Avas12a1 reduced the signal to the background level of 40 nM IRDye800-IgG.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2%20optical+rodentia)]

Virostko et al. (12) performed in vivo NIR fluorescence imaging studies of IRDye800-Avas12a1 (0.5 nmol/mouse) in mice bearing VEGFR-2-negative 4T1 murine breast tumor. Images were obtained longitudinally up to 40 h after intravenous injection. IRDye800-Avas12a1 exhibited peak signal intensity at 24 h with a gradual washout. Significant fluorescence was observed in the liver, kidneys and tumor area. On the other hand, IRDye800-IgG showed similar biodistribution in the liver and kidneys but the tumor area did not display any fluorescence signal over the background. The tumor/muscle ratio of IRDye800-Avas12a1 was significantly (P < 0.0001) higher (1.69 ± 0.08, n = 20) than that of IRDye800-IgG (0.93 ± 0.07, n = 6) at 24 h after injection. In a separated study, NIR imaging was performed in mice bearing the 4T1 tumor treated with 40 mg/kg sunitinib daily for 5 days. Sunitinib (http://google2.fda.gov/search?q=Sunitinib&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=10) is an oral, small-molecule, multi-targeted receptor tyrosine kinase (http://en.wikipedia.org/wiki/Receptor_tyrosine_kinase) inhibitor that was approved by the U.S. Food and Drug Administration for the treatment of renal cell carcinoma (http://en.wikipedia.org/wiki/Renal_cell_carcinoma). Sunitinib inhibits tumor angiogenesis and tumor growth. Fluorescence signal of IRDye800-Avas12a1 in the tumors of sunitinib-treated mice (2.356 ± 0.074, n = 10) was significantly (P < 0.002) reduced as compared with the tumors of saline treated mice (1.832 ± 0.1284, n = 9) at 24 h after injection. Tumor sizes were reduced by 28 ± 4% with sunitinib as compared with saline. Immunohistochemical analysis of untreated tumor sections showed that VEGFR-2 expression was confined to the endothelial cells. Sunitinib treatment reduced the VEGFR2 expression in the endothelial cells of the tumor sections (P < 0.027).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2%20optical+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2%20optical+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2%20optical+human)]

No publication is currently available.

## NIH Support

P50 CA098131, P50 CA128323, T32 EB001628, T32 EB003817, U24 CA126588, K25 CA127349, P30 CA068485

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
5 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
6 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
7 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
8 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
9 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
10 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
11 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
12 Virostko J., Xie J., Hallahan D.E., Arteaga C.L., Gore J.C., Manning H.C. (2009). A molecular imaging paradigm to rapidly profile response to angiogenesis-directed therapy in small animals. Mol Imaging Biol.